# ^125^I-Labeled single-chain monoclonal antibody, NS4F5, that targets the GlcNS6S-IdoA2S motif of heparan sulfate proteoglycans for the in vivo imaging of peripheral amyloidosis

Chemical name: | ^125^I-Labeled single-chain monoclonal antibody, NS4F5, that targets the GlcNS6S-IdoA2S motif of heparan sulfate proteoglycans for the in vivo imaging of peripheral amyloidosis
Abbreviated name: | [^125^I]-NS4F5
Synonym:
Agent Category: | Antibody
Target: | GlcNS6S-IdoA2S motif of heparan sulfate proteoglycans
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planer imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Peripheral%20amyloidosis&cmd=DetailsSearch)]

Peripheral amyloidosis (http://www.nlm.nih.gov/medlineplus/amyloidosis.html) is the extracellular deposition of insoluble protein fibrils in various organs of animals, including humans, and these deposits are considered to be biomarkers for diseases such as Alzheimer’s disease (AD), light chain amyloidosis (AL), etc (1). The fibrils are made up of disease-specific aggregated proteins or peptides (e.g., Aβ peptides for AD, light chains for AL or multiple myeloma, and reactive amyloidosis (AA)) that incorporate heparin sulfate proteoglycans (HSPG; heparin belongs to the heparan sulfate family of proteoglycans that contain the (GlcNS6S-IdoA2S)_3_ motif)) and the serum amyloid P component (SAP) within their structure during disease progression. A characteristic feature of the protein fibrils is that the constituent proteins form a secondary cross-β pleated sheet structure that is resistant to proteolytic digestion (for structural details, see Goldsbury et al. (2)). In addition, clinical symptoms of amyloidosis in a patient are influenced by the degree to which an organ is involved in the disease (3).The HSPG contain diverse types of oligosaccharides that are sulfated on the hydroxyl moieties to varying degrees, and these hypersulfated structures are distinct, are found specifically in the amyloid deposits, and differ from one another depending on the organ where they are located (4). In addition, the HSPG contain stretches of the disaccharide GlcNS6S-IdoA2S (HS^NS4F5^; these motifs are abundantly found in heparin, but have limited presence in the HS of normal tissues) that inhibit cell proliferation and induce apoptosis but do not affect the attachment of cells to collagen I (5). Because the HSPG in the amyloids are hypersulfated compared to the proteoglycans in normal tissues, HSPG are considered to be suitable for the detection of amyloids with imaging techniques and to diagnose and monitor amyloidosis progression and to determine the prognosis for a patient with amyloidosis (1).

Whole-body scintigraphy with radioiodinated SAP is commonly used in Europe for the detection of amyloidosis in the various parts of the body, but this technique is not approved by the United States Food and Drug Administration for clinical use in United States because the SAP used to generate the tracer is isolated from human sources (1). In an attempt to develop an amyloid imaging agent that would not require the use of human materials, Wall et al. showed that a ^125^I-labeled synthetic heparin-binding peptide, p5, could be used with single-photon emission computed tomography (SPECT) to detect amyloid deposits in H2/huIL-6 transgenic mice with severe systemic AA amyloidosis (AA mice) (1). In another study, Wall et al. evaluated the use of ^125^I-labeled single chain (scFv) antibodies (Abs) directed against HS for the detection of amyloids in AA mice that are prone to develop amyloidosis at ~4–5 months of age as described elsewhere (6). Among these radioiodinated scFv Abs, NS4F5, which binds specifically to HS^NS4F5^ (5), has been determined to be the most suitable for the noninvasive imaging of amyloids in the transgenic animals (6).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Amyloid+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/search/open/condition=%22Amyloidosis%22) related to amyloidosis

Amyloidosis in Online Mendelian Inheritance in Man Database (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=amyloidosis)

Protein (http://www.ncbi.nlm.nih.gov/protein/AAA35526.1) sequence of human amyloid

Crystal structures (http://www.ncbi.nlm.nih.gov/structure?term=Human%20amyloid%20proteins) of human amyloid proteins

Symptoms, diagnosis, and treatment of amyloidosis (http://www.cedars-sinai.edu/Patients/Health-Conditions/Amyloidosis.aspx?gclid=CJbMzuybm6wCFYTe4AodsyAo1g) (at Cedars-Sinai Medical Center, LA)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-heparin%20antibodies%20production&cmd=DetailsSearch)]

Anti-HS scFv Abs (HS4C3, NS4F5, HS4E4, and the chondroitin sulfate–binding scFv Ab GD3G7) were produced and purified as described by Wall et al. (6). The antibodies were labeled with ^125^I using the chloramine-T method and the labeled Abs were purified with gel filtration on Sepharose Aca 44 gel in 0.01 M sodium phosphate (pH 7.6) and 0.15 M sodium chloride containing 5 mg/mL bovine serum albumin. The radiochemical purity (RCP) of the labeled Abs was evaluated with SDS/PAGE and phosphorimaging (6). The radiochemical yield, RCP, and specific activity of the labeled Abs were 50.9 ± 10.0%, 96.6 ± 2.8%, and 25–40 μCi/nmol protein, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-heparin%20antibodies%20in%20vitro%20studies&cmd=DetailsSearch)]

The binding specificities of the various Abs to the chemical groups in HS (for HS4C3, NS4F5, and HS4E4) and chondroitin sulfate (for GD3G7) were established with the ELISA technique and have been described by Wall et al. (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-heparin%20antibodies%20rodentia&cmd=DetailsSearch)]

The biodistribution of the ^125^I-labeled Ab fragments (scFv) was investigated in amyloidosis induced in AA mice as described by Wall et al. (6). The amyloid deposits were found primarily in the liver, spleen, and pancreas of these animals. Wild-type (WT) mice from the same colony (identified by genotyping; non-transgenic) were used as controls for this study. The animals (n = 3 animals/Ab) were injected with ~7.40 MBq (~200 μCi; ~25 μg) of the labeled Abs through the lateral tail vein and euthanized 1–4 h later by isoflurane inhalation overdose. SPECT/Computed tomography (CT) images of the animals were subsequently acquired, and all major tissues were collected for biodistribution measurement (data were expressed as percent of injected dose per gram tissue (% ID/g)) and microautoradiography. At 1 h postinjection (p.i.), no difference in the uptake of radioactivity in the various organs of the AA and the WT mice was apparent with any Ab. However, because the AA mice are known to have slow clearance of ScFv Abs through the kidneys due to the amyloid pathology, the tissue/muscle (T/M) ratios were calculated from the data. Among the different Abs, only NS4F5 showed at least a two-fold higher T/M ratio in the liver, spleen, and kidneys of AA mice compared to the same organs from the WT animals. No other labeled Ab showed a similar increase in the ratio except HS4E4, which had a more than two-fold T/M ratio in the kidneys of the AA mice compared to the WT animals. In general, the kidneys (9%–13% ID/g) and the stomach (11%–22% ID/g) of the WT mice showed the highest concentration of radioactivity, and the investigators attributed this to renal catabolism and dehalogination of the radioiodinated Ab followed by sequestering of the ^125^I iodide to the stomach (this organ has a high concentration of iodide symporters). At 4 h p.i., most of the radioactivity from the Abs was associated with the liver and kidneys in the AA mice (these organs have large amounts of amyloid deposits), and this was confirmed with SDS/PAGE analysis of the various tissues of animals treated with ^125^I-NS4F5 (the labeled scFv chains ran midway on the gel, whereas the ^125^I iodide ran just ahead of the dye front; the Rf values for the two fractions were not reported). A similar analysis of tissues obtained from the WT mice showed that the radioactivity was present largely as free radioiodide except in the kidney, which had some label bound to the scFv.

For SPECT/CT imaging, the AA and WT mice (n = 3 animals/Ab) were injected with the radioiodinated scFvs as described above, and the images were acquired while the rodents were under anesthesia (6). At 1 h p.i., images of the WT mice injected with the different Abs showed that radioactivity was present mainly in the stomach while trace amounts of the label were detected in the kidneys. In addition, from the images it was evident that only ^125^I-NS4F5 had a distinct distribution in the AA mice because the liver and spleen of these animals showed a higher uptake of radioactivity compared to the organs of the WT animals. This indicated that the scFv NS4F5 was probably the most suitable for the imaging of amyloid deposits in the mice. No blocking studies were reported.

To confirm that ^125^I-NS4F5 was indeed the most suitable scFv Ab for the imaging of amyloid deposits, a second biodistribution and SPECT/CT imaging study was performed with this tracer (6). The AA and WT mice (n = 3 mice/group/time point) were injected with 4.5 MBq (120 μCi) ^125^I-NS4F5, and SPECT/CT images were acquired from the animals under anesthesia at 1, 4, and 24 h p.i. Images acquired at 1 h p.i. showed that the radioactivity was present mainly in the liver and spleen of the AA mice, whereas in the WT mice the label was observed primarily in the stomach and the thyroid. At 4 h p.i., the images of the AA and the WT mice looked similar, thus indicating that the labeled scFv was lost from the amyloid deposits in the AA mice and the WT animals at this time point. At 1 h p.i. the thyroid of the WT and the AA animals showed a similar accumulation of the label, but at 4 h p.i the amount of radioactivity in the AA thyroid was ~5 fold (~2%ID/g) that of the WT mice. From this observation, the investigators concluded that 1 h p.i. was the best time point to image the amyloid deposits in these animals. By 24 h p.i., little radioactivity remained in the animals (AA and WT) to acquire any images (6). Biodistribution measurements of the different tissues at 1, 4, and 24 h confirmed the SPECT/CT imaging data. At 1 h p.i., the AA mice had more than two-fold higher radioactivity in the liver, spleen, and kidneys compared to the same organs from the WT animals. By 4 h p.i., this difference increased to approximately four-fold, and by 24 h p.i., although most of the label had cleared from the organs of the AA and the WT mice, the AA/WT ratio for most organs were similar but remained >1. The investigators suggested that this was probably due to a defective renal function, which leads to slow clearance of the label from the AA animals.

On the basis of results obtained from the studies described above, the investigators concluded that scFv NS4F5 requires further improvement before it can be used as an agent for imaging amyloid deposits (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-heparin%20antibodies%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-heparin%20antibodies%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-heparin%20antibodies%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies reported in this chapter were supported by National Institute of Diabetes and Digestive and Kidney Diseases Award R01DK079984.

## References

1 Wall J.S., Richey T., Stuckey A., Donnell R., Macy S., Martin E.B., Williams A., Higuchi K., Kennel S.J. (2011). In vivo molecular imaging of peripheral amyloidosis using heparin-binding peptides. Proc Natl Acad Sci U S A.
2 Goldsbury C., Baxa U., Simon M.N., Steven A.C., Engel A., Wall J.S., Aebi U., Muller S.A. (2011). Amyloid structure and assembly: insights from scanning transmission electron microscopy. J Struct Biol.
3 Perfetto F., Moggi-Pignone A., Livi R., Tempestini A., Bergesio F., Matucci-Cerinic M. (2010). Systemic amyloidosis: a challenge for the rheumatologist. Nat Rev Rheumatol.
4 Ori A., Wilkinson M.C., Fernig D.G. (2008). The heparanome and regulation of cell function: structures, functions and challenges. Front Biosci.
5 Smits N.C., Kurup S., Rops A.L., ten Dam G.B., Massuger L.F., Hafmans T., Turnbull J.E., Spillmann D., Li J.P., Kennel S.J., Wall J.S., Shworak N.W., Dekhuijzen P.N., van der Vlag J., van Kuppevelt T.H. (2010). The heparan sulfate motif (GlcNS6S-IdoA2S)3, common in heparin, has a strict topography and is involved in cell behavior and disease. J Biol Chem.
6 Wall, J.S., T. Richey, A. Stuckey, R. Donnell, A. Oosterhof, T.H. van Kuppevelt, N.C. Smits, and S.J. Kennel, SPECT imaging of peripheral amyloid in mice by targeting hyper-sulfated heparan sulfate proteoglycans with specific scFv antibodies. Nucl Med Biol, 2011